# Gold/silica nanoparticles with a near-infrared fluorescent and PEGylated paramagnetic lipid coating

Chemical name: | Gold/silica nanoparticles with a near-infrared fluorescent and PEGylated paramagnetic lipid coating
Abbreviated name: | Au-SiFluPaLCs
Synonym:
Agent Category: | Nanoparticles
Target: | Non-targeted
Target Category:
Method of detection: | Multimodal imaging (magnetic resonance imaging, optical imaging, computed tomography)
Source of signal / contrast: | Gd, Cy5.5, and gold (Au)
Activation: | No
Studies: | - In vitro; - Rodents | No structure is available.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=multimodal%20imaging%20agent)]

The gold/silica nanoparticle with a near-infrared (NIR) fluorescent and PEGylated paramagnetic lipid coating, abbreviated as Au-SiFluPaLCs, is a trimodal imaging agent that has been developed by van Schooneveld et al. for combined magnetic resonance imaging (MRI), computed tomography (CT), and optical imaging (1).

The idea of using multiple modalities in a single imaging session comes from the fact that imaging modalities with high sensitivity have relatively poor resolution, while those with high resolution have relatively poor sensitivity (2, 3). Integration of multiple modalities in imaging would combine the advantages of each modality and allow better characterization of diseases and disease processes (4). Development of hybrid imaging technology has also triggered great effort in the development of multimodal imaging agents to boost the benefits of hybrid instrument technology (5, 6).

In principle, the synthesis of multimodal agents is similar to that of single-mode agents (6). A large molecule is usually necessary for efficient labeling and delivery of multiple reporters. Intensively investigated large molecules include liposomes, dendrimers, polymers, and endogenous nanoparticles (6, 7). In the case of liposomes, reporters are either encapsulated in the aqueous interior space or incorporated into the lipid bilayer (1, 8). The latter approach usually results in an improved ionic relaxivity of the MRI metals. In the development of multimodal agents, questions arise from the multistep conjugations that often lead to a low chemical yield. The presence of different molecules on the same nanoparticle surface may interfere with the targeting capabilities and the subsequent intracellular uptake of the agents. The optimization of multimodal imaging agents is more challenging in terms of immunogenicity, toxicity, specificity, interference with biological processes, and accumulation in target organs (5, 6).

van Schooneveld et al. and Koole et al. synthesized a series of multimodal imaging agents by coating silica particles with a dense monolayer of PEGylated paramagnetic lipids without the use of coupling agents (1, 8, 9). The presence of a dense lipid layer around the inorganic core renders these particles stable in aqueous dispersion and bioapplicable. The lipid coating also allows for conjugation of target-specific molecules at the surface of nanoparticles. These agents include Q-SiPaLCs, RGD-conjugated Q-SiPaLCs, and Au-SiFluPaLCs. Of these agents, Au-SiFluPaLCs was synthesized as a trimodal contrast agent for combined MRI, CT, and optical imaging (1). This trimodal agent is composed of a gold/silica particle core with a NIR fluorescent and PEGylated paramagnetic lipid coating. The electron-dense gold core enables its detection with CT, while the paramagnetic lipids generate the MRI signal and the NIR dye Cy5.5 allows for optical imaging. The results obtained with Au-SiFluPaLCs have shown that the trimodal agent effectively labels phagocytotic cells in vitro and mouse liver cells in vivo. This agent can be a useful tool in a multitude of applications, including cell tracking and targeted molecular imaging (1). This chapter summarizes the data obtained with Au-SiFluPaLCs. Another chapter in MICAD summarizes the data obtained with Q-SiPaLCs (http://www.ncbi.nlm.nih.gov/books/NBK5330/).

### Related Resource Links:

Multimodal imaging agents in MICAD (http://www.ncbi.nlm.nih.gov/books/?term=multimodality+AND+micad%5bbook%5d&view=chapter&p%24a=&p%24l=PBooksLayout&p%24st=books)

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=%22van%20Schooneveld%20MM%22%5bAuthor%5d)]

van Schooneveld et al. described the synthesis of Au-SiFluPaLCs in detail (1). Briefly, gold nanocrystals were first cultivated to 66 ± 8 nm and then coated with a silica shell (~11 nm thick) via the polyvinylpyrrolidone method to an average particle diameter of 88 ± 9 nm. The silica surface was further coated with paramagnetic, dye-conjugated, and PEGylated lipids by dissolving the following components in chloroform: hydrophobic gold/silica particles, Cy5.5-conjugated 1,2-distearoyl-sn-glycero-3-phosphoethanolamine-N-(methoxy(poly(ethylene glycol))-2000) (PEG-DSPE), and 1,2-distearoyl-sn-glycero-3-phosphoethanolamine-N-[maleimide-(poly(ethylene glycol))2000] (Mal-PEG-DSPE), and gadolinium diethylenetriamine pentaacetic acid di(stearylamide) (Gd-DTPA-DSA). The molar ratio of PEG-DSPE, Mal-PEG-DSPE, and Gd-DTPA-DSA was 0.4/0.1/0.5 in the lipids. The mixture was then added dropwise to hot physiological buffer to rapidly evaporate the chloroform, which resulted in a micellar lipid coating of the gold/silica particles. The NIR dye Cy5.5 was chosen to minimize re-absorption of the emission (698 nm) by the plasmon absorption band of the gold cores (558 nm).

The presence of the dense lipid layer around the inorganic particle core resulted in a shelf-life of at least 3 months. With negative stain transmission electron microscopy (TEM), a hydrophobic layer of ~2 nm could be found on the lipid-coated particles. The hydrodynamic diameter of the lipid-coated particles was ~108 nm, 20 nm larger than the average of 88 ± 9 nm, as estimated with TEM and laser-based dynamic light scattering (1, 8).

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=%22van%20Schooneveld%20MM%22%5bAuthor%5d)]

The sensitivity of Au-SiFluPaLCs for detection with optical imaging, MRI (1.5 T), and CT (110 keV) was determined with concentration–signal curve analysis (1). The fluorescence intensity correlated with the agent concentration in a nonlinear pattern due to the re-absorption of emitted light by the gold nanocrystal cores at higher particle concentrations. The MRI and CT signals, however, increased linearly with particle concentration in the nanomolar regime. The ionic longitudinal relaxivity r_1_ of the Gd incorporated in the lipid layer was found to be 14.0 mM^-1^s^-1^. The total number of lipids/particle was 40,000, of which half carried Gd-DTPA-DSA. For CT, the slope of the concentration–signal curve was found to be 23 Hounsfield units (HU) per gram of gold per liter of solution.

The in vitro imaging potential of Au-SiFluPaLCs was tested by labeling murine macrophage J774A.1 cells (n = ~1 × 10^6^) (1). The cells were incubated for 24 h with 1.3 nM Au-SiFluPaLCs. Microscopy showed fluorescence in cells as a result of the nanoparticles containing Cy5.5. MRI (9.4 T) and CT (110 keV) showed strong contrast enhancement for the cell pellets as compared with the cell pellets of untreated macrophages.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=%22van%20Schooneveld%20MM%22%5bAuthor%5d)]

The in vivo MRI and CT imaging of mouse livers (n = 2) were performed after intravenous administration of Au-SiFluPaLCs at a dose of 0.15 nmol/kg weight (1). T1-Weighted MRI (9.4 T) of the mouse liver at 24 h after injection showed a 24% mean intensity enhancement when normalized to muscle signal. CT showed a 50% mean X-ray attenuation increase when liver images were compared before agent administration (37.95 ± 1.96 HU) and 24 h after agent administration (56.75 ± 2.95 HU).

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20%28dog%20OR%20rabbit%20OR%20pig%20OR%20sheep%29)]

No references are currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20%28primate%20NOT%20human%29)]

No references are currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20human)]

No references are currently available.

## References

1 van Schooneveld M.M., et al. (2010). A fluorescent, paramagnetic and PEGylated gold/silica nanoparticle for MRI, CT and fluorescence imaging. Contrast Media Mol Imaging.
2 Cherry S.R. (2006). Multimodality in vivo imaging systems: twice the power or double the trouble?. Annu Rev Biomed Eng.
3 Cherry S.R. (2009). Multimodality imaging: beyond PET/CT and SPECT/CT. Semin Nucl Med.
4 Jennings L.E., Long N.J. (2009). 'Two is better than one'--probes for dual-modality molecular imaging. Chem Commun (Camb).
5 Lee S., Chen X. (2009). Dual-modality probes for in vivo molecular imaging. Mol Imaging.
6 Louie A. (2010). Multimodality imaging probes: design and challenges. Chem Rev.
7 Alric C., et al. (2008). Gadolinium chelate coated gold nanoparticles as contrast agents for both X-ray computed tomography and magnetic resonance imaging. J Am Chem Soc.
8 Koole R., et al. (2008). Paramagnetic lipid-coated silica nanoparticles with a fluorescent quantum dot core: a new contrast agent platform for multimodality imaging. Bioconjug Chem.
9 van Schooneveld M.M., et al. (2008). Improved biocompatibility and pharmacokinetics of silica nanoparticles by means of a lipid coating: a multimodality investigation. Nano Lett.